# [^18^F]α/γ-Fluorobenzylamine-folate

Chemical name: | [^18^F]α/γ-Fluorobenzylamine-folate
Abbreviated name: | [^18^F]α/γ-FBA-folate, [^18^F]FBA-folate
Synonym:
Agent category: | Compound
Target: | Putative folate receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate)]

Folic acid is a water-soluble B vitamin (1) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1-5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher affinity (dissociation constant (K_d_) = 0.5 nM) receptor that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate-binding protein (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20-50%). Activated macrophages, but not resting macrophages, have been also found to have folate receptor (3).

Several folate-based conjugates (^111^In-DTPA-folate, ^99m^Tc-EC-folate and ^68/67/66^Ga-DF-folate (http://www.ncbi.nlm.nih.gov/books/NBK23092/)) have been studied in tumor imaging (4-7). Bettio et al. (8) reported a synthesis of 18F-labeled folate by a reaction of [^18^F]4-fluorobenzylamine (FBA) with the α- and γ-carboxyl groups of folic acid. [18F]α/γ-FBA-folate is being developed as a positron emission tomography (PET) agent for detection of folate receptors in vivo.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in OMIM (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20synthesis)]

Bettio et al. (8) coupled folic acid with [^18^F]FBA to yield a 4:1 mixture of [^18^F]γ-FBA-folate and

[^18^F]α-FBA-folate with radiochemical yields of 15-44% and specificity activity up to 24 GBq/μmol (0.65 Ci/μmol). [^18^F]FBA was prepared by a two-step reaction by standard nucleophilic radiofluorination of 4-cyano-N,N,-trimethylanilinium trifluoromethane sulfonate to form 4-[^18^F]-benzonitrile and reduction of the nitrile functional group by LiAlH_4_ to the amino functionality with radiochemical yields of 8-13%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20in%20vitro)]

The human nasopharyngeal carcinoma KB-31 cell line has putative folate receptors as determined by [^3^H]folate binding studies in cultures (8). The mean IC_50_ values for α-FBA-folate, γ-FBA-folate and folate were 71 ± 8, 62 ± 6 and 41 nM, respectively. Therefore, the α- and γ-FBA-folate have comparable binding affinity to that of native folic acid.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20rodentia)]

Bettio et al. (8) performed biodistribution studies of [^18^F]α/γ-FBA-folate in nude mice bearing the KB-31 tumor xenografts. The organ with the highest accumulation was the kidneys (40.65%ID/g), followed by the tumor (6.65%ID/g), duodenum (5.01%ID/g), and liver (2.37%ID/g) at 125 min after [^18^F]α/γ-FBA-folate injection. Very high radioactivity was found in bile, urine, and faces. Pretreatment with folic acid (200 μg/mouse) reduced [^18^F]α/γ-FBA-folate accumulation by 80% in the tumor and 97% in the kidneys.

The whole body distribution of [^18^F]α/γ-FBA-folate was also assessed by PET imaging from 75 to 120 min after injection. The highest activity concentrations were visualized in the gallbladder, urinary bladder, and parts of the intestines. Moderate accumulation was observed in the kidneys, tumors, and liver. The accumulation of [^18^F]α/γ-FBA-folate was heterogeneous within the tumor, with higher radioactivity in the tumor rim. The accumulation of [^18^F]α/γ-FBA-folate in the tumor and kidneys was completely blocked by folic acid pretreatment.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20folate%20and%20human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
4 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
5 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
6 Mathias C.J., Wang S., Low P.S., Waters D.J., Green M.A. (1999). Receptor-mediated targeting of 67Ga-deferoxamine-folate to folate-receptor-positive human KB tumor xenografts. Nucl Med Biol.
7 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.
8 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and Preclinical Evaluation of a Folic Acid Derivative Labeled with 18F for PET Imaging of Folate Receptor-Positive Tumors. J Nucl Med.